# N-2-(4-[^18^F]-Fluorobenzamido)ethylmaleimide coupled to cysteine-tagged on the C- or N-terminal of exendin-4

Chemical name: | N-2-(4-[^18^F]-Fluorobenzamido)ethylmaleimide coupled to cysteine-tagged on the C- or N-terminal of exendin-4
Abbreviated name: | [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4
Synonym:
Agent Category: | Peptide
Target: | Glucogon-like peptide 1 receptor (GLP-1R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=insulinoma&cmd=DetailsSearch)]

Pancreatic neuroendocrine tumors (PNET) are rare and are classified as nonfunctional or functional as discussed in detail by Batcher et al. (1). Nonfunctional PNETs usually grow in size and eventually cause a mass effect in the organ, whereas functional tumors secrete one (or more) active hormones and are subclassified on the basis of the hormone secreted by the cells constituting the tumor (e.g., insulinomas (secrete insulin), glucagonomas (secrete glucagon), somatostatinomas (secrete somatostatin), etc.). Insulinomas are the most common PNETs observed in the clinic, and biochemical tests of these patients show that the individuals have fasting hypoglycemia along with hyperinsulinoma (elevated levels of insulin) (1). Complete surgical resection of the tumor is considered to be the most suitable treatment and cure for the patient (2). Most insulinomas are small and benign, and they exist as single lesions. Imaging techniques such as computed tomography (CT), magnetic resonance imaging (MRI), and endoscopic ultrasound (EUS) are often used to detect and determine the location of these tumors on the pancreas (3). However, the preoperative detection of these lesion with noninvasive imaging is difficult because the techniques are either unable to distinguish the tumor from the normal parenchymal tissue in the pancreas (e.g., CT), are expensive (e.g., MRI), or are invasive and operator-dependent (e.g., EUS) (3, 4).

Investigators have shown that insulinomas characteristically express high levels of glucagon-like peptide 1 (GLP-1) receptors (GLP-1R), and radiolabeled GLP-1–like ligands have been developed and evaluated for the detection of these PNETs (5). Although GLP-1 is the natural ligand for the GLP-1R, a major drawback of using this peptide to detect the lesions is that it is rapidly inactivated (half-life, ~2 min) by proteolytic enzymes while in circulation. As a consequence, investigators identified ^111^In-labeled exendin-4 or its analogs (exendin is a peptide of 39 amino acids that has a 54% homology with GLP-1, acts as an agonist of the GLP-1R, and is not inactivated by proteolytic enzymes) for the detection of insulinomas in Rip1Tag2 mice that have spontaneous insulinoma (6) and in humans (4). In another study, EM3106B, an analog of GLP-1 that contains lactam bridges, was labeled with ^18^F by coupling it with N-2-(4-[^18^F]-fluorobenzamido)ethylmaleimide ([^18^F]-FBEM), and the labeled compound was successfully used with positron emission tomography (PET) to detect subcutaneous insulinomas in nude mice (7). As an extension of the earlier work, structural analogs of exendin-4 were conjugated with [^18^F]FBEM for labeling with ^18^F, and the biodistribution of [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4 was studied in mice bearing INS-1 cell xenograft tumors (for structural details of the compounds, see the Synthesis section below) (5). The radiolabeled compounds were also evaluated with PET to detect tumors that overexpressed GLP-1R in these mice.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Exendin-4+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GLP-1R) related to GLP-1R

Gene information (http://www.ncbi.nlm.nih.gov/gene/2740) regarding human GLP-1R (Gene ID: 2740)

Glucagon-like peptide 1 (http://omim.org/entry/138030) in Online Mendelian Inheritance in Man Database (OMIM)

Mouse GLP-1R (http://www.genome.jp/dbget-bin/www_bget?mmu:14652) in Kyoto Encyclopedia of Genes and Genomes Database (KEGG)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22170321%5Buid%5D&cmd=DetailsSearch)]

Because exendin-4 does not contain a cysteine residue in its native structure, the peptide was modified with a C-terminal cysteine ([Cys^0^]-exendin-4) or an N-terminal cysteine ([Cys^40^]-exendin-4) to permit site-specific labeling of the analogs with [^18^F]FBEM (5). [Cys^0^]-exendin-4 and [Cys^40^]-exendin-4 were prepared commercially using solid-phase peptide synthesis procedures. The radiochemical synthesis of [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4 has been described by Kiesewetter et al. (5). The radiochemical yield of the labeling reactions for both the tracers was 34.3 ± 3.4%, and the radiochemical purity of the labeled compounds at the time of preparation was >96% as determined with high-performance liquid chromatography (HPLC). The specific activity of the preparations was reported to be 45.51 ± 16.28 GBq/μmol (1.23 ± 0.44 Ci/μmol; n = 7 preparations).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22170321%5Buid%5D&cmd=DetailsSearch)]

Using [^125^I]GLP-1 as the ligand in a competition assay with INS-1 cells (Western blot analysis showed that these cells had a high expression of GLP-1R), the binding affinities of unlabeled FBEM-[Cys^0^]-exendin-4 and FBEM-[Cys^40^]-exendin-4 were determined to be 1.88 ± 0.075 nM and 1.22 ± 0.049 nM, respectively (5). The 50% inhibition concentration values for GLP-1, FBEM-[Cys^0^]-exendin-4, and FBEM-[Cys^40^]-exendin-4 were reported to be 5.33 ± 0.053 nM, 2.99 ± 0.0056 nM, and 1.11 ± 0.057 nM, respectively. This indicated that, among the different ligands of GLP-1R investigated in this study, FBEM-[Cys^40^]-exendin-4 exhibited the maximum affinity for the receptor.

The uptake, internalization, and efflux of [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4 were investigated with INS-1 cells (5). Both tracers had similar uptake values in the cells (~0.5% of added dose), and after 2 h of incubation, 80% of the radioactivity had been internalized by the cells. Both probes were reported to have a gradual and biphasic efflux from the cells.

In another study, unlabeled FBEM-[Cys^40^]-exendin-4 was incubated with mouse serum and human plasma, respectively, for up to 1 h at 37°C (5). At the end of the incubation, a radio-HPLC analysis of the mixture showed that 20% and 32% of the compound was adsorbed to the serum and the plasma proteins, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22170321%5Buid%5D&cmd=DetailsSearch)]

The biodistribution of [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4 was studied in mice bearing INS-1 cell xenograft tumors or MDA-MB-435 cell xenograft tumors (do not express the GLP-1R; negative controls) as described by Kiesewetter et al. (5). The animals (n = 6 mice/group; under anesthesia) were injected with 3.44 ± 0.26 MBq (~100 μCi) of each tracer through the tail vein, and microPET images were acquired at 1 h and 2 h postinjection (p.i.). From the images it was determined that the radioactivity uptake values with the ^18^F-labeled [Cys^0^]-and [Cys^40^] analogs of exendin-4 in the INS-1 cell tumors at 1 h p.i. were 7.20 ± 1.26% injected dose per gram tissue (% ID/g) and 25.25 ± 3.39% ID/g, respectively. With [^18^F]FBEM-[Cys^0^]-exendin-4, the accumulation of radioactivity in the MD-MB-435 tumors was 0.67 ± 0.06% ID/g during the same period. At 2 h p.i., the amount of label in the tumors was ~4% ID/g and ~20% ID/g with [^18^F]FBEM-[Cys^0^]-exendin-4 and [^18^F]FBEM-[Cys^40^]-exendin-4, respectively. Ex vivo quantification of radioactivity in the different tissues of the animals showed that the tumor/kidney and tumor/liver ratios with [^18^F]FBEM-[Cys^0^]-exendin-4 were 0.48 and 7.4, respectively, and with [^18^F]FBEM-[Cys^40^]-exendin-4 these ratios were 4.8 and 39.9, respectively.

For blocking studies, the mice (n = 4 animals) were injected with 200 μg (~45 nmol) unlabeled [Cys^0^]-exendin-4 or [Cys^40^]-exendin-4 10 min before either [^18^F]FBEM-[Cys^0^]-exendin-4 or [^18^F]FBEM-[Cys^40^]-exendin-4 were administered to the animals (5). An ex vivo analysis of the major tissues from the animals showed that the radioactivity from both the tracers was reduced by >87% (P < 0.05) in the INS-1 tumors, pancreas, and lungs. With the [Cys^40^] isomer, there was a 52% (P < 0.05) inhibition of uptake in the intestine, but the liver, kidneys, and muscle showed a >49% increase in accumulation of radioactivity. However, the investigators did not explain the increased uptake of label observed in these organs.

From these studies, the investigators concluded that the [Cys^40^] isomer was a candidate for further development as a GLP-1R imaging agent because, compared with [^18^F]FBEM-[Cys^0^]-exendin-4, a higher uptake of radioactivity in the tumor was observed with [^18^F]FBEM-[Cys^40^]-exendin-4 and this labeled analog generated better tumor/nontarget tissue ratios in the rodents (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-Cys40-exendin-4%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-Cys40-exendin-4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-Cys40-exendin-4%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies presented in this chapter were supported by the Intramural Research Program of the National Institute of Biomedical Imaging and Bioengineering, National Institutes of Health.

## References

1 Batcher E., Madaj P., Gianoukakis A.G. (2011). Pancreatic neuroendocrine tumors. Endocr Res.
2 Mathur A., Gorden P., Libutti S.K. (2009). Insulinoma. Surg Clin North Am.
3 McAuley G., Delaney H., Colville J., Lyburn I., Worsley D., Govender P., Torreggiani W.C. (2005). Multimodality preoperative imaging of pancreatic insulinomas. Clin Radiol.
4 Wild D., Macke H., Christ E., Gloor B., Reubi J.C. (2008). Glucagon-like peptide 1-receptor scans to localize occult insulinomas. N Engl J Med.
5 Kiesewetter D.O., Gao H., Ma Y., Niu G., Quan Q., Guo N., Chen X. (2012). (18)F-radiolabeled analogs of exendin-4 for PET imaging of GLP-1 in insulinoma. Eur J Nucl Med Mol Imaging.
6 Wild D., Behe M., Wicki A., Storch D., Waser B., Gotthardt M., Keil B., Christofori G., Reubi J.C., Macke H.R. (2006). [Lys40(Ahx-DTPA-111In)NH2]exendin-4, a very promising ligand for glucagon-like peptide-1 (GLP-1) receptor targeting. J Nucl Med.
7 Gao H., Niu G., Yang M., Quan Q., Ma Y., Murage E.N., Ahn J.M., Kiesewetter D.O., Chen X. (2011). PET of insulinoma using 18F-FBEM-EM3106B, a new GLP-1 analogue. Mol Pharm.